# ^111^In-DTPA-Bz-NH-SA-K(IR-783-S-Ph-CO)-c(CGRRAGGSC)NH_2_

Chemical name: | ^111^In-DTPA-Bz-NH-SA-K(IR-783-S-Ph-CO)-c(CGRRAGGSC)NH_2_
Abbreviated name: | ^111^In-DLIA-IL11Rα
Synonym:
Agent Category: | Peptide
Target: | Interleukin-11 (IL-11) receptor
Target Category: | Receptor binding
Method of detection: | Optical, near-infrared (NIR) fluorescence and SPECT, gamma planar imaging
Source of signal: | IR-783 and ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=15341755), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=24430217) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=3589&ordinalpos=3&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about IL-11.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DLIA-IL11R+111In)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal fluorescence background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity because of low fluorescence background, as well as high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in small animals (4, 5).

Interleukin-11 (IL-11) is a multifunctional growth factor for blood cells and their precursors (6). IL-11 receptor high-affinity binding complex consists of a low-affinity IL-11 ligand-binding α-chain (IL-11Rα) and a signal-transduction β-chain (gp 130). IL-11 and IL-11Rα are involved in breast cancer development and progression (7, 8). Arap et al. (9) reported that the cyclic nonapeptide c(CGRRAGGSC) was capable of binding specifically to IL-11Rα. Wang et al. (10) reported the development of a multimodality imaging agent, ^111^In-DTPA-Bz-NH-SA-K(IR-783-S-Ph-CO)-c(CGRRAGGSC)NH_2_ (^111^In-DLIA-IL11Rα), for imaging IL-11Rα expression on breast tumors: single-photon emission computed tomography (SPECT) used ^111^In-DTPA-Bz-NH-SA and NIR imaging used IR-783-S-Ph-CO.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DLIA-IL11R+111In+Synthesis)]

In the report by Wang et al. (10), IR783-S-Ph-CONHS was conjugated to the ω-NH_2_ group of Lys in DTPA-Bz-NH-SA-K-c(CGRRAGGSC)NH_2_ by incubation overnight. Unlabeled DLIA-IL11Rα in 0.1 N sodium acetate was mixed with an aqueous solution of ^111^InCl_3_ for 30 min to form ^111^In-DLIA-IL11Rα. Specific activity and radiochemical yield were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DLIA-IL11R+111In+In+Vitro)]

Wang et al. (10) performed cell-binding assays with In-DLIA-IL11Rα using the human breast cancer cell line MDA-MB-231 (positive for IL-11Rα). High fluorescence intensity was observed on the cell surface of MDA-MB-231 cells after incubation for 10 min at 37°C. Binding of In-DLIA-IL11Rα to IL-11–activated MAD-MB-231 cells was enhanced compared to nonstimulated cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DLIA-IL11R+111In+Rodentia)]

Wang et al. (10) performed a preliminary study of ^111^In-DLIA-IL11Rα in nude mice bearing MDA-MB-231 tumors (7–8 mm in diameter) using the whole-body fluorescence detection system and SPECT/CT. ^111^In-DLIA-IL11Rα (2 nmol/mouse) was injected intravenously into nude mice bearing tumors showing a higher fluorescence signal in the tumor than in the muscle 24 h after injection. The kidneys also displayed a distinct fluorescence signal. The SPECT/CT images also confirmed the accumulation of ^111^In-DLIA-IL11Rα in the tumor and kidneys 24 h after injection. Ex vivo gamma counting showed that the tumor/muscle, liver/muscle, and kidney/muscle ratios were 2.12, 2.62, and 10.42, respectively. No blocking experiment was performed. The authors mentioned that the optimal dose and biodistribution of ^111^In-DLIA-IL11Rα remain to be determined.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DLIA-IL11R+111In+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DLIA-IL11R+111In+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DLIA-IL11R+111In+human)]

No publication is currently available.

## NIH Support

R01 EB003132

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Robeson W., Dhawan V., Belakhlef A., Ma Y., Pillai V., Chaly T., Margouleff C., Bjelke D., Eidelberg D. (2003). Dosimetry of the dopamine transporter radioligand 18F-FPCIT in human subjects. J Nucl Med.
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 Kawashima I., Takiguchi Y. (1992). Interleukin-11: a novel stroma-derived cytokine. Prog Growth Factor Res.
7 Sotiriou C., Lacroix M., Lespagnard L., Larsimont D., Paesmans M., Body J.J. (2001). Interleukins-6 and -11 expression in primary breast cancer and subsequent development of bone metastases. Cancer Lett.
8 Hanavadi S., Martin T.A., Watkins G., Mansel R.E., Jiang W.G. (2006). Expression of interleukin 11 and its receptor and their prognostic value in human breast cancer. Ann Surg Oncol.
9 Arap W., Kolonin M.G., Trepel M., Lahdenranta J., Cardo-Vila M., Giordano R.J., Mintz P.J., Ardelt P.U., Yao V.J., Vidal C.I., Chen L., Flamm A., Valtanen H., Weavind L.M., Hicks M.E., Pollock R.E., Botz G.H., Bucana C.D., Koivunen E., Cahill D., Troncoso P., Baggerly K.A., Pentz R.D., Do K.A., Logothetis C.J., Pasqualini R. (2002). Steps toward mapping the human vasculature by phage display. Nat Med.
10 Wang W., Ke S., Kwon S., Yallampalli S., Cameron A.G., Adams K.E., Mawad M.E., Sevick-Muraca E.M. (2007). A new optical and nuclear dual-labeled imaging agent targeting interleukin 11 receptor alpha-chain. Bioconjug Chem.